# Malachite green-isothiocyanate-polyethylene glycol-gold nanoparticles conjugated with scFv anti-EGFR B10 antibody

Chemical name: | Malachite green isothiocyanate-polyethylene glycol-gold nanoparticles conjugated with scFv anti-EGFR B10 antibody
Abbreviated name: | MGITC-AuNPs-scFvB10
Synonym:
Agent Category: | Metal
Target: | EGFR, HER1
Target Category: | Antibody-antigen binding
Method of detection: | Optical, surface-enhanced Raman scattering
Source of signal: | Malachite green
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence (NIRF) imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Hainfeld et al. (3) performed experiments in mice using gold nanoparticles (AuNPs; 1.9 nm in diameter, ~50 kDa) as a computed tomography contrast agent to enhance imaging contrast in the vasculature, kidneys, and tumor tissue in mice. No physiological complications were observed in the mice for up to a year. James et al. (4) showed that gold nanoshells (110 nm in diameter) coated with polyethylene glycol (PEG) had no toxic effects in mice for up to 28 days. PEG is found to minimize nonspecific adsorption of proteins onto nanoparticles and to reduce their uptake by the liver (5). Surface-enhanced Raman scattering (SERS) involves surface plasmons of silver and gold as excited by a NIR laser (785 nm), and the resulting electric fields cause other nearby molecules (reporter molecules) to become Raman active (6, 7). The result is amplification of the Raman signals (by up to 10^14^), allowing detection and identification of single molecules. Qian et al. (8) found that SERS PEG-AuNPs (60–80 nm) are >200 times brighter (NIR signal) than quantum dots on a particle-to-particle basis. A single-chain anti-EGFR B10 antibody fragment (~25 kDa) consisting of the variable V_H_ and V_L_ domains for antigen binding (scFvB10) was conjugated to SERS nanoparticles (MGITC-AuNPs-scFvB10) for tumor imaging in a small animal model. The reporter molecules are malachite green isothiocyanate (MGITC). MGITC-AuNPs-scFvB10 has electronic transitions at 633 nm or 785 nm.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast)]

Qian et al. (8) reported the preparation MGITC-AuNPs-scFvB10. A solution of 3–4 µM of MGITC was added slowly to a rapidly stirred gold colloid solution. After 10 min, a solution of thio-PEG (10 µM) was added dropwise to the MGITC-AuNP solution. The MGITC-AuNP solution was washed and isolated by centrifugation. The core size of each MGITC-AuNP was ~60 nm with >30,000 copies of thio-PEG (5 kDa). For protein conjugation, a solution of thio-PEG-COOH (1 µM) was added slowly to another freshly prepared MGITC-AuNP solution. After 15 min, a large excess of thio-PEG was added to coat the area not covered by the thio-PEG-COOH. A solution of ethyl dimethylaminopropyl carbodiimide and sulfo-N-hydroxysuccinimide was added to activate the carboxyl groups of PEG-COOH on the MGITC-AuNPs. The activated nanoparticles were incubated with scFv B10 antibody (11.2 nmol) for 20 h. MGITC-AuNPs-scFvB10 was isolated and purified by centrifugation and membrane filtration to remove the unreacted antibody. There were ~600 copies of scFv B10 antibody/nanoparticle; there were 1.4–1.5 × 10^4^ MGITC molecules/nanoparticle. MGITC-AuNPs-scFvB10 had a hydrodynamic diameter of ~80 nm. MGITC-AuNPs-scFvB10 has electronic transitions at 633 nm for NIRF imaging and 785 nm for NIR SERS imaging; therefore, MGITC-AuNPs-scFvB10 is a multimodal agent. Another reporter dye (diethylthiatricarbocyanine (DTTC)) conjugated with AuNPs-scFvB10 (DTTC-AuNPs-scFvB10) was also prepared similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20in%20vitro)]

Qian et al. (8) performed cell-binding assays with DTTC-AuNPs-scFvB10 using human head-and-neck carcinoma Tu866 (HER1-positive) and non-small cell lung carcinoma NCI-H520 (HER1-negative) cell lines. SERS measurements at 30 min of incubation with DTTC-AuNPs-scFvB10 (15 pM) showed that Tu866 cells exhibited strong SERS signals, whereas H520 cells showed little or no signal. Pretreatment of Tu866 cells with a ten-fold excess of scFvB10 abrogated the binding of DTTC-AuNPs-scFvB10 to the cells. No signal was obtained after incubation of Tu866 cells with DTTC-AuNPs-IgG (nonspecific antibody) or DTTC-AuNPs (control).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20rodentia)]

Qian et al. (8) performed studies in which MGITC-AuNPs (0.05 pmol) were injected subcutaneously in a nude mouse (1–2 mm under the skin and 1 cm deep in muscle). NIR Raman spectroscopy (full width at half maximum = 1–2 nm) was used to measure SERS spectra at the two locations at 3 and 21 s after injection. The highly resolved SERS signals obtained were identical to the reference MGITC-AuNPs spectrum, although the intensities were one- to two-fold lower. It was estimated that SERS signals could be detected as deep as 2 cm into tissue. In another experiment, either MGITC-AuNPs-scFvB10 or MGITC-AuNP (460 pmol) was injected intravenously into nude mice (n = 4) bearing a Tu866 xenograft tumor (3 mm in diameter). NIR Raman spectroscopy of the tumor and liver in vivo was performed at 5 h. There were substantial differences in the tumor signal intensities between the targeted and non-targeted nanoparticles. In contrast, the SERS signal intensities were similar in the liver. The tumor SERS signal intensities of targeted nanoparticles were ~three-fold greater than those of the liver and stayed in the tumor for >24 h. The biodistribution of the nanoparticles was measured by inductively coupled plasma-mass spectroscopy at 5 h after injection. The excised tissue with the highest MGITC-AuNPs-scFvB10 accumulation was the spleen (40 ppm), followed by the liver (14 ppm) and the tumor (9 ppm). There was minimal accumulation in the kidney, muscle, and lung. MGITC-AuNPs and MGITC-AuNPs-IgG had similar biodistribution values as compared with MGITC-AuNPs-scFvB10, with the exception of the tumor (<1 ppm for MGITC-AuNPs and MGITC-AuNPs-IgG). AuNPs were taken up by the reticuloendothelial system and phagocytes in the liver and spleen. Transmission electron microscopy images of the tumor cells showed intracellular clusters of MGITC-AuNPs-scFvB10 in intracellular endosomes and lysosomes. On the other hand, the liver Kupffer cells and spleen macrophages showed intracellular accumulation of single nanoparticles in these organelles. No signs of sickness were observed in the mice injected with these nanoparticles for up to 2–3 months. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanoparticles%20X-ray%20contrast%20and%20human)]

No publication is currently available.

## NIH Support

U54 CA119338, P50 CA128613

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hainfeld J.F., Slatkin D.N., Focella T.M., Smilowitz H.M. (2006). Gold nanoparticles: a new X-ray contrast agent. Br J Radiol.
4 James W.D., Hirsch L.R., West J.L., O'Neal P.D., Payne J.D. (2007). Application of INAA to the build-up and clearance of gold nanoshells in clinical studies in mice. Journal of Radioanalytical and Nuclear Chemistry.
5 Otsuka H., Nagasaki Y., Kataoka K. (2003). PEGylated nanoparticles for biological and pharmaceutical applications. Adv Drug Deliv Rev.
6 Freeman R.G., Grabar K.C., Allison K.J., Bright R.M., Davis J.A., Guthrie A.P., Hommer M.B., Jackson M.A., Smith P.C., Walter D.G., Natan M.J. (1995). Self-Assembled Metal Colloid Monolayers: An Approach to SERS Substrates. Science.
7 Nie S., Emory S.R. (1997). Probing Single Molecules and Single Nanoparticles by Surface-Enhanced Raman Scattering. Science.
8 Qian X., Peng X.H., Ansari D.O., Yin-Goen Q., Chen G.Z., Shin D.M., Yang L., Young A.N., Wang M.D., Nie S. (2008). In vivo tumor targeting and spectroscopic detection with surface-enhanced Raman nanoparticle tags. Nat Biotechnol.